# Magnetic iron microbeads coupled with HEA-125 monoclonal antibody against epithelial cell adhesion molecule

Chemical name: | Magnetic iron microbeads coupled with HEA-125 monoclonal antibody against epithelial cell adhesion molecule
Abbreviated name: | EpCAM microbeads
Synonym: | CD326 microbeads
Agent Category: | Nanoparticles
Target: | Epithelial cell adhesion molecule (EpCAM)
Target Category: | Adhesion molecules
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=epithelial%20cell%20adhesion%20molecule%20and%20imaging)]

Magnetic iron microbeads coupled with HEA-125 monoclonal antibody against the epithelial cell adhesion molecule (EpCAM), abbreviated as EpCAM microbeads, have been developed primarily for the positive selection or depletion of EpCAM-positive cells (1, 2). McClelland et al. have demonstrated the feasibility of cell tracking with magnetic resonance imaging (MRI) after the hepatic progenitor cells are labeled with EpCAM microbeads (1).

Superparamagnetic iron oxide (SPIO)-based agents have been intensively tested for use in cell tracking with MRI in both preclinical and clinical situations (3, 4). SPIO particles provide a strong change in signal per unit of metal in T2-weighted images without a significant effect on labeled cells and host (3, 5). For efficient cell labeling, SPIO particles are generally coated with low-molecular-weight polymers or dendrimers leading to clusters of electron-dense crystal cores covered with the polymer or dendrimer. Surface coating increases the stability of SPIO particles and allows further chemical modification of the particles with targeting ligands. Cell tracking studies have shown that the migration and homing capabilities of SPIO-labeled cells can be monitored in vivo over days to months (3, 4, 6).

Nevertheless, there are still many challenges to overcome before MRI cell tracking can be considered a robust technique in preclinical settings or in clinical applications (3, 7). MRI detects the presence of SPIO contrast agents, regardless of whether SPIO particles remain in the relevant cells, are lost to the extracellular matrix, or are transferred to other cells. It is still not possible to use MRI to discriminate live cells from dead cells or relevant cells from phagocytes. Detection sensitivity also becomes an issue when cells actively divide and migrate, in which case the SPIO labels are quickly divided among daughter cells to levels that are undetectable with MRI. In vivo quantification of the cell number is more challenging because of the contrast agent dilution during cell division, contrast agent transfer to others cells, other sources of iron in tissue, and technical limitations (4, 7).

McClelland et al. addressed the problem of contrast agent dilution in MRI cell tracking by using EpCAM microbeads as the label (1). The human EpCAM, also known as CD326 or epithelial-specific antigen, is a cell-surface antigen and is found on hepatic progenitor cells, including human hepatic stem cells (hHpSCs) and hepatoblasts (hHBs), on liver cancer stem cells, and on proliferating epithelial cells in other tissues (8-10). The human EpCAM is not expressed in animal cells. McClelland et al. studied the labeling of hHpSCs with EpCAM microbeads in vitro, ex vivo, and in vivo and imaged the labeled cells with MRI (1). The investigators demonstrated that the hHpSCs could be labeled with EpCAM microbeads before or after transplantation, and the transplanted hHpSCs could be monitored and counted repeatedly in the same host by injection of the label just prior to MRI (1).

### Related Resource Links:

- Chapters on MRI cell tracking in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=cell%20tracking%20AND%20micad%5bbook%5d)
- The protein (http://www.ncbi.nlm.nih.gov/protein/?term=epithelial+cell+adhesion+molecule) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=epithelial%20cell%20adhesion%20molecule) information of EpCAM
- Articles on EpCAM in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=epithelial%20cell%20adhesion%20molecule)
- Datasheets of the CD326 MicroBeads (http://www.miltenyibiotec.com/download/datasheets_en/90/DS130_061_101.pdf)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20890665)]

EpCAM microbeads (brand name, CD326 MicroBeads) are commercially available and have an overall diameter of 50–100 nm (1). The magnetic iron microbeads were coupled with HEA-125 monoclonal antibodies against the human EpCAM. The amount of monoclonal antibodies per microbead was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20890665)]

Cell labeling with EpCAM microbeads was analyzed after the hHpSCs, prepared from human fetal livers, were exposed to the beads at a concentration of 10 µl EpCAM microbeads per 10^7^ cells in 100 µl buffer for 40 min at 4°C (1). After labeling, excess microbeads were washed, and the cells were cultured for 24 more hours. Transmission electron microscopy, scanning electron microscopy, and dispersive x-ray imaging confirmed the cell internalization and cell surface attachment of the EpCAM microbeads. The labeling efficiency. i.e., the amount of Fe or beads per cell, and the effect of labeling on cell function were not reported.

Detection feasibility with MRI was tested with labeled and unlabeled cell aggregates embedded in 1% agarose on 35-mm Petri dishes (1). In contrast to the controls without cells and with unlabeled cells, gel that contained labeled cells showed conspicuously large clusters of signal voids of varying sizes, which were attributed to the cell aggregates of varying sizes. Detection sensitivity was not reported.

McClelland et al. established an MRI method for both in vitro and in vivo quantification of the cell number (1). Three-dimensional aggregates of the hHpSCs were generated by placing cells in culture dishes. The radius, diameter, and area of the cell aggregates were measured under microscopy as well as with MRI, assuming that a single hHpSC has a radius of ~8 μm and that the descendents of hHpSCs (the hHBs) have a single-cell radius of ~11 μm. A strong correlation (r^2^ = 0.99) was obtained between the cell aggregate radii obtained under microscopy and those measured with MRI. The cell aggregates appeared larger (64% larger in this case) in MRI than in actuality because the influence of the magnetic beads that give rise to the MRI contrast usually extends beyond their physical boundary. On the basis of the cell number and cell aggregate radius measured under microscopy, equations for the cell count (N) in terms of MRI-observed aggregate radius (r_MRI_) were then established as N ≈ 104 + 4.2E – 4r^3^_MRI_ for spherical aggregates and N ≈ 104 + 1.0E – 4V_MRI_ for non-spherical aggregates, where the E represents the power of 10 and the V_MRI_ is the volume of the MRI region of interest. Cell numbers could be computed directly from the in vivo MRI images with the use of these equations (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20890665)]

McClelland et al. first tested the MRI detection and quantification of labeled cells in situ with a 7-T scanner (1). Livers from Sprague-Dawley rats (n = 3) were isolated and perfused with buffer. Labeled and unlabeled hHpSCs (~2 × 10^6^) were transplanted directly into the livers through portal vein catheterization, and the organs were imaged immediately after transplantation. Intensity voids from the aggregates of labeled cells were observed throughout the liver. The labeled cell aggregates had an average radius of 133.4 µm, which corresponded to an average cell count of 1.1 × 10^2^.

McClelland et al. then analyzed the post-transplantation cell labeling efficiency and quantified the cell number (1). Labeled and unlabeled hHpSCs (2 × 10^6^) were injected into the liver of SCID/NOD mice (n = 16) through the splenic vasculature that is connected directly to the liver. In this way, the majority of the cells went directly to the liver. Eight hours later, the mice were euthanized, and the livers were excised, perfusion-fixed, and imaged. For the controls injected without labeled hHpSC cells, injected with microbeads alone, and injected with unlabeled hHpSCs (n = 4 mice/group), MRI images of the perfused liver appeared as a homogeneous background except for the hyperintense branching pathways near the liver center that correspond to the hepatic sinusoids. For the mice injected with unlabeled hHpSCs but subsequently given microbeads through the tail vein on days 6 and 18 after transplantation, a total of four and seven hHpSC aggregates were detected as hypointense foci in the MRI image slices from days 6 and 18, respectively. In the image slice from day 18, the cell aggregates were clearly located near the large sinusoidal pathways of the liver, which is consistent with the fact that cells transplanted into the liver via the portal vein migrate through sinusoidal pathways before integrating into the liver tissue. The number of cells in the aggregates was calculated with the equations described in In Vitro Studies. More aggregates and up to 12 times more cells were found on day 18 than on day 6, indicating post-transplantation cell proliferation.

In summary, McClelland et al. demonstrated a method for in vivo MRI cell tracking that enabled noninvasive monitoring of hHpSCs after transplantation (1). The cells could be labeled before or after transplantation with EpCAM microbeads that can distinguish transplanted cells from host cells. In this study, however, the background in MRI imaging was limited by using xenogeneic transplants of human hepatic progenitors into animals, by using EpCAM antigen expressed only on the human cells, and by perfusing liver tissues to remove blood before imaging. The accuracy of the cell number quantification from the in vivo images was not further validated (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 McClelland, R., E. Wauthier, T. Tallheden, L.M. Reid, and E. Hsu, In Situ Labeling and Magnetic Resonance Imaging of Transplanted Human Hepatic Stem Cells. Mol Imaging Biol, 2010
2 Bulte J.W., Douglas T., Witwer B., Zhang S.C., Strable E., Lewis B.K., Zywicke H., Miller B., van Gelderen P., Moskowitz B.M., Duncan I.D., Frank J.A. (2001). Magnetodendrimers allow endosomal magnetic labeling and in vivo tracking of stem cells. Nat Biotechnol.
3 Arbab A.S., Liu W., Frank J.A. (2006). Cellular magnetic resonance imaging: current status and future prospects. Expert Rev Med Devices.
4 Bulte J.W. (2009). In vivo MRI cell tracking: clinical studies. AJR Am J Roentgenol.
5 Himmelreich U., Dresselaers T. (2009). Cell labeling and tracking for experimental models using magnetic resonance imaging. Methods.
6 Kiessling, F., Noninvasive cell tracking. Handb Exp Pharmacol, 2008(185 Pt 2): p. 305-21.
7 Srinivas M., Aarntzen E.H., Bulte J.W., Oyen W.J., Heerschap A., de Vries I.J., Figdor C.G. (2010). Imaging of cellular therapies. Adv Drug Deliv Rev.
8 van der Gun B.T., Melchers L.J., Ruiters M.H., de Leij L.F., McLaughlin P.M., Rots M.G. (2010). EpCAM in carcinogenesis: the good, the bad or the ugly. Carcinogenesis.
9 Trzpis M., McLaughlin P.M., de Leij L.M., Harmsen M.C. (2007). Epithelial cell adhesion molecule: more than a carcinoma marker and adhesion molecule. Am J Pathol.
10 Munz M., Baeuerle P.A., Gires O. (2009). The emerging role of EpCAM in cancer and stem cell signaling. Cancer Res.